# 2-(4-(4-[^18^F]Fluoro-butyl)-benzylsulfanyl)-3-methyl-chromen-4-one

Chemical name: | 2-(4-(4-[^18^F]Fluoro-butyl)-benzylsulfanyl)-3-methyl-chromen-4-one
Abbreviated name: | [^18^F]RP1005
Synonym:
Agent category: | Compound
Target: | Mitochondrial complex I (MCI)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1005)]

Lipophilic cations are capable of passing through biological membranes by passive diffusion into the cytoplasm and mitochondria of cells in response to large negative plasma and mitochondrial membrane potentials. ^99m^Tc-2-Methoxyisobutylisonitrile (^99m^Tc-MIBI) and ^99m^Tc-tetrofosmin are delocalized lipophilic cations, which are rapidly taken up into cells driven by metabolic demand and membrane potential (1-4). They are used as myocardial-perfusion single-photon emission computed tomography agents and as tumor-imaging agents. However, the high accumulation of Tc tracers in the lung and liver may interfere with the detection of flow abnormalities in the myocardium. More recently, positron emission tomography (PET) imaging has emerged as an alternative approach to evaluate myocardial blood flow with the use of positron-emitting radionuclides (e.g., ^82^RbCl, ^13^NH_3_, and H_2_^15^O). However, the majority of these radiotracers exhibit short physical half-lives (<10 min). Lipophilic cations such as [^11^C]triphenylmethylphosphonium ([^11^C]TPMP) (5) and 4-[^18^F]fluorobenzyl-triphenylphosphonium ([^18^F]FBnTP) have been investigated as PET agents for myocardial and tumor imaging (6).

Mitochondrial complex I (MCI) of the mammalian electron transfer chain is composed of at least 43 protein subunits, of which seven are encoded by mitochondrial DNA (7). MC-I catalyzes the transfer of electrons from NADH to ubiquinone and translocates protons from the mitochondrial matrix to the intermembrane space to generate ATP and thus the energy supply of the cell. MC-I may also play direct roles in the mitochondrial permeability transition and in cell death pathways. Myocardium has a high mitochondrial content because of high energy usage. 2-(4-(4-[^18^F]Fluoro-butyl)-benzylsulfanyl)-3-methyl-chromen-4-one ([^18^F]RP1005) has been found to be a potent MC-I inhibitor with a hydrophobic heterocyclic chromone (8) and its use as a PET agent for imaging myocardium is being studied.

### Related Resource Links:

- Chapters in MICAD (MCI (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=Mitochondrial%20complex+AND+micad%5Bbook%5D))
- Gene information in NCBI (MCI (http://www.ncbi.nlm.nih.gov/gene/291))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MCI (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=252010))
- Clinical trials (MCI (http://www.clinicaltrials.gov/ct2/results?term=Mitochondrial+complex+I+))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1005+synthesis)]

[^18^F]RP1005 was prepared as described by Yu et al. (8). [^18^F]Fluoride/Kryptofix 2.2.2/K_2_CO_3_ and the tosylate precursor were heated in acetonitrile for 30 min at 90°C, followed by high-performance liquid chromatography purification. Total synthesis time was 90 min. Radiochemical purity was >90%, with specific activities of 27.8–55.5 GBq/µmol (0.75–1.5 Ci/µmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1005%20and%20in%20vitro)]

Yu et al. (8) reported that RP1005 inhibited NADH oxidation by bovine heart submitochondrial particles with a 50% inhibition concentration (IC_50_) value of 14.4 nM. The IC_50_ value of the known MC-I inhibitor rotenone was 18.2 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1005%20and%20rodentia)]

Yu et al. (8) performed ex vivo biodistribution studies of [^18^F]RP1005 in rats (n = 12). [^18^F]RP1005 accumulated mainly in the heart, with 2.28 ± 0.12% injected dose/g (ID/g) and 1.81 ± 0.17% ID/g at 15 min and 60 min after injection, respectively. Retention of [^18^F]RP1005 in the heart was good, with little washout. The heart/blood, heart/lung, heart/liver, and heart/femur ratios were 20.1, 10.1, 2.2, and 4.5 at 60 min after injection, respectively. The uptake in the femur was 0.40% ID/g at 60 min, indicating little defluorination of [^18^F]RP1005. For comparison, heart accumulation of ^99m^Tc-sestamibi was 2.0% ID/g at 60 min, with a heart/lung ratio of 5.9 at 60 min after injection. PET imaging showed that [^18^F]RP1005 accumulated mainly in the heart and liver with low accumulation in the lung. Good myocardial images were observed at 25–35 min after injection, with little interference from the lung or liver at 55–60 min. No blocking experiment was performed. The first pass extraction efficiency was not addressed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F%20RP1005+and+(dog+or+pig+or+sheep+or+rabbit))]

Yu et al. (8) performed PET imaging studies of [^18^F]RP1005 in rabbits (n = 6). [^18^F]RP1005 accumulated mainly in the myocardium within minutes after injection, with some interference from the lung and liver at 5–15 min after injection. Retention of [^18^F]RP1005 in the heart was good and exhibited little washout, whereas the retention was much lower in the liver. Accumulation of [^18^F]RP1005 in the heart was clearly visualized at 65 min after injection, with some interference from the lung and liver accumulation of [^18^F]RP1005.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1005%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20RP1005%20and%20human)]

No publication is currently available.

## References

1 Chernoff D.M., Strichartz G.R., Piwnica-Worms D. (1993). Membrane potential determination in large unilamellar vesicles with hexakis(2-methoxyisobutylisonitrile)technetium(I). Biochim Biophys Acta.
2 Chiu M.L., Kronauge J.F., Piwnica-Worms D. (1990). Effect of mitochondrial and plasma membrane potentials on accumulation of hexakis (2-methoxyisobutylisonitrile) technetium(I) in cultured mouse fibroblasts. J Nucl Med.
3 Molteni S.N., Seregni E., Botti C., Martinetti A., Ferrari L., Crippa F., Bombardieri E. (1999). The breast cancer cell line MCF7 as a model of 99mTc-SestaMIBI, 99mTc-tetrofosmin and 99mTc-Medronate incorporation. Anticancer Res.
4 Younes A., Songadele J.A., Maublant J., Platts E., Pickett R., Veyre A. (1995). Mechanism of uptake of technetium-tetrofosmin. II: Uptake into isolated adult rat heart mitochondria. J Nucl Cardiol.
5 Krause B.J., Szabo Z., Becker L.C., Dannals R.F., Scheffel U., Seki C., Ravert H.T., Dipaola A.F., Wagner H.N. (1994). Myocardial perfusion with [11C]methyl triphenyl phosphonium: measurements of the extraction fraction and myocardial uptake. J Nucl Biol Med.
6 Madar I., Ravert H.T., Du Y., Hilton J., Volokh L., Dannals R.F., Frost J.J., Hare J.M. (2006). Characterization of Uptake of the New PET Imaging Compound 18F-Fluorobenzyl Triphenyl Phosphonium in Dog Myocardium. J Nucl Med.
7 Lenaz G., Fato R., Genova M.L., Bergamini C., Bianchi C., Biondi A. (2006). Mitochondrial Complex I: structural and functional aspects. Biochim Biophys Acta.
8 Yu M., Guaraldi M., Kagan M., Mistry M., McDonald J., Bozek J., Yalamanchili P., Hayes M., Azure M., Purohit A., Radeke H., Casebier D.S., Robinson S.P. (2009). Assessment of 18F-labeled mitochondrial complex I inhibitors as PET myocardial perfusion imaging agents in rats, rabbits, and primates. Eur J Nucl Med Mol Imaging.